# ^111^In-Labeled anti-CD44v6 chimeric monoclonal antibody U36

Chemical name: | ^111^In-Labeled anti-CD44v6 chimeric monoclonal antibody U36
Abbreviated name: | ^111^In-cMAb U36
Synonym: | ^111^In-U36
Agent Category: | Chimeric monoclonal antibody
Target: | Adhesion molecule CD44v6
Target Category: | Antibody-antigen binding
Method of detection: | Single-photon emission computed tomography; planar gamma imaging
Source of Signal/Contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click here for protein and nucleotide information (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=960&log$=databasead&logdbfrom=protein) on CD44.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CD44v6+antibody)]

CD44 is a member of the family of cell adhesion molecules that is known to promote cell migration and survival during cancer metastasis (1). The mouse CD44 gene contains ~20 exons, of which 10 are variants that are alternatively spliced for incorporation into the molecule to yield several CD44 variants (CD44v). The different CD44v forms have been reviewed elsewhere (2). The various CD44v molecules are involved in modulating a variety of cellular processes including cell migration and localization in the diverse organs, thereby promoting cancer metastasis (3). Among these variants, the variant containing domain 6 of the exons (CD44v6) has been specifically implicated in tumorigenesis and tumor cell migration (4). In normal tissue CD44v6 is expressed in a subset of epithelial cells, and it is found in most squamous cell carcinomas and some adenocarcinomas, but CD44v6 is seldom observed in tumors that have a nonepithelial origin (4). Also, CD44v6 was reported to have higher expression compared with the epidermal growth factor receptor in samples obtained from head and neck squamous cell carcinoma (HNSCC) tumors of patients (5).

Because of its high expression in HNSCC, CD44v6 has been targeted with a monoclonal antibody (MAb), designated U36, for the diagnosis of this cancer in humans (6, 7). The biodistribution of U36 was investigated after being labeled with radioactive technetium, and it was reported that the labeled MAb could detect all primary tumors of HNSCC, but the micro-tumors or tumor nodes with necrosis, keratin, or fibrin were not visible by imaging (7). This MAb was also evaluated in two clinical trials for the treatment of HNSCC after labeling with radioactive rhenium (^186^Re), but the ^186^Re dose was not sufficient to kill the small tumors or the decimated single cells from this cancer (8). U36 was also labeled with radioactive astatine (^211^At) and iodine (^131^I) and evaluated for the in vitro treatment of HNSCC cells; the ^211^At-conjugated MAb was shown to be more lethal to the HNSCC cells than the ^131^I-labeled homolog (9). In another study, the ^211^At-labeled MAb was shown to decrease or stabilize the volume of xenograft tumors in nude mice (10). U36 labeled with ^124^I or ^131^I has also been evaluated for the detection of xenograft tumors in nude mice, and the selective uptake of both labels by the tumors was confirmed with positron emission tomography (11, 12).

The U36 MAb was recently labeled with radioactive indium (^111^In), and its in vitro characteristics were investigated with the use of SCC-9 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1629&Template=cellBiology) cells derived from HNSCC (13). The use of 111In to label the cMAb was considered because of its longer intracellular retention probably due to the formation of charged catabolites that do not pass through the membrane easily. The biodistribution of the ^111^In-labeled chimeric MAb (cMAb) was also studied in nude mice bearing xenograft SCC-9 cell tumors (14). Imaging with the mice was also performed with single-photon emission computed tomography 72 h after administration of the ^111^In-labeled cMAb (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+MAb+U36+synthesis)]

The hybridomas that were used to produce the U36 MAb were developed as described by Schrijvers et al. (15). A chimeric version of the MAb (cMAb U36) was prepared as described by Brakenhoff et al. (16). The cMAb U36 was obtained in citrate buffer and separated with size-exclusion chromatography (SEC) on a NAP-5 column. It was then lyophilized and stored at -20°C until required (13).

Sandstrom et al. labeled cMAb U36 with ^111^In with the use of N-[(R)-2-amino-3-(p-isothiocyanato-pentyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-N,N,N’,N”,N”-pentaacetic acid (CHX-A”-DTPA) as a chelator (14). The cMAb was mixed with CHX-A”-DTPA in a molar ratio of 5:1 in borate buffer (pH 9.15), and the reaction was allowed to occur for 2 h at 37°C. The conjugated cMAb was then separated from unreacted CHX-A”-DTPA with SEC on a NAP-5 column in acetate buffer (pH 5.5). For labeling, the conjugated cMAb was mixed with ^111^In, and the mixture was incubated at room temperature for 30 min. The labeled cMAb (^111^In-cMAb U36) was separated from the reaction components with SEC as described above on a column equilibrated with phosphate-buffered saline. The labeling yield was reported to be 70% to 80%. The specific activity and stability of the labeled cMAb was not reported by the investigators (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+MAb+U36+in+vitro)]

The in vitro receptor binding of ^111^In-cMAb U36 was characterized by using SCC-9 cells (13). The uptake and retention of ^111^In-cMAb U36 was also studied in the SCC-9 cells at 4° and 37°, C respectively. The dissociation constant for ^111^In-cMAb U36 was determined to be 1.3 ± 0.3 × 10^-8^ M. Cellular uptake of the labeled cMAb was observed to plateau at ~4 h after exposure at both 4° and 37°, C respectively. In the presence of unlabeled cMAb, the uptake was minimal and remained constant during this period. To determine cellular retention of the labeled cMAb, the cells were first exposed to the labeled cMAb for 8 h and then washed (wash buffer was not specified) to remove any unbound radioactivity. Complete growth medium was then added to the cells, and the amount of radioactivity retained by the cells was monitored for 16 h. The cells were observed to lose the radioactivity gradually, and ~40% of the initial radioactivity was retained after 8 h of incubation, indicating that the labeled cMAb was internalized by the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+cMAb+U36+rodentia)]

The biodistribution of ^111^In-cMAb U36 was studied in nude mice bearing xenograft tumors of SCC-9 cells (14). The animals were injected with the labeled cMAb through the tail vein and killed at 6, 24, 48, 72, and 168 h after injection (n = 3 animals/time point). The various organs were harvested, and the incorporated radioactivity was measured. At 48 h after administration, the highest uptake of radioactivity was observed in the liver (13.9 ± 1.47% injected dose/g tissue (% ID/g)), followed by the spleen (10.52 ± 2.81% ID/g), lungs (7.12 ± 4.29% ID/g), skin (5.85 ± 0.64% ID/g), and heart (4.72 ± 0.67% ID/g). The kidneys had the maximum uptake (7.70 ± 0.22% ID/g) at 24 h after injection. The radioactivity decreased in the organs from the peak as a function of time. The tumors had a five-fold higher accumulation of the label compared with blood (54.7 ± 16.6 versus 10.91 ± 1.06) at 168 h after injection of the labeled cMAb. The tumor/blood ratio increased from 0.24 ± 0.10 at 6 h to 4.45 ± 1.35 at 168 h after injection of the radioactivity.

For scintigraphic imaging, two mice bearing SCC-9 xenograft tumors were injected with ^111^In-cMAb U36, and images were collected after 72 h. From the images, the uptake values were determined to be 7.9% ID/g (mouse 1; tumor weight, 230 mg) and 11.0% ID/g (mouse 2; tumor weight, 60 mg), respectively.

### Other Non-Primate Mammals

[PubMed]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+cMAb+U36+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+cMAb+U36+humans)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Naor D., Wallach-Dayan S.B., Zahalka M.A., Sionov R.V. (2008). Involvement of CD44, a molecule with a thousand faces, in cancer dissemination. Semin Cancer Biol.
2 Ponta H., Sherman L., Herrlich P.A. (2003). CD44: from adhesion molecules to signalling regulators. Nat Rev Mol Cell Biol.
3 Wallach-Dayan S.B., Rubinstein A.M., Hand C., Breuer R., Naor D. (2008). DNA vaccination with CD44 variant isoform reduces mammary tumor local growth and lung metastasis. Mol Cancer Ther.
4 Heider K.H., Kuthan H., Stehle G., Munzert G. (2004). CD44v6: a target for antibody-based cancer therapy. Cancer Immunol Immunother.
5 Nestor M., Ekberg T., Dring J., van Dongen G.A., Wester K., Tolmachev V., Anniko M. (2007). Quantification of CD44v6 and EGFR expression in head and neck squamous cell carcinomas using a single-dose radioimmunoassay. Tumour Biol.
6 de Bree R., Roos J.C., Plaizier M.A., Quak J.J., van Kamp G.J., den Hollander W., Snow G.B., van Dongen G.A. (1997). Selection of monoclonal antibody E48 IgG or U36 IgG for adjuvant radioimmunotherapy in head and neck cancer patients. Br J Cancer.
7 de Bree R., Roos J.C., Quak J.J., den Hollander W., Snow G.B., van Dongen G.A. (1995). Radioimmunoscintigraphy and biodistribution of technetium-99m-labeled monoclonal antibody U36 in patients with head and neck cancer. Clin Cancer Res.
8 Colnot D.R., Quak J.J., Roos J.C., van Lingen A., Wilhelm A.J., van Kamp G.J., Huijgens P.C., Snow G.B., van Dongen G.A. (2000). Phase I therapy study of 186Re-labeled chimeric monoclonal antibody U36 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
9 Nestor M., Persson M., van Dongen G.A., Jensen H.J., Lundqvist H., Anniko M., Tolmachev V. (2005). In vitro evaluation of the astatinated chimeric monoclonal antibody U36, a potential candidate for treatment of head and neck squamous cell carcinoma. Eur J Nucl Med Mol Imaging.
10 Cheng J., Ekberg T., Engstrom M., Nestor M., Jensen H.J., Tolmachev V., Anniko M. (2007). Radioimmunotherapy with astatine-211 using chimeric monoclonal antibody U36 in head and neck squamous cell carcinoma. Laryngoscope.
11 Verel I., Visser G.W., Vosjan M.J., Finn R., Boellaard R., van Dongen G.A. (2004). High-quality 124I-labelled monoclonal antibodies for use as PET scouting agents prior to 131I-radioimmunotherapy. Eur J Nucl Med Mol Imaging.
12 Fortin M.A., Salnikov A.V., Nestor M., Heldin N.E., Rubin K., Lundqvist H. (2007). Immuno-PET of undifferentiated thyroid carcinoma with radioiodine-labelled antibody cMAb U36: application to antibody tumour uptake studies. Eur J Nucl Med Mol Imaging.
13 Nestor M., Andersson K., Lundqvist H. (2007). Characterization of 111In and 177Lu-labeled antibodies binding to CD44v6 using a novel automated radioimmunoassay. J. Mol. Recognit.
14 Sandstrom K., Nestor M., Ekberg T., Engstrom M., Anniko M., Lundqvist H. (2008). Targeting CD44v6 Expressed in Head and Neck Squamous Cell Carcinoma: Preclinical Characterization of an In-Labeled Monoclonal Antibody. Tumour Biol.
15 Schrijvers A.H., Quak J.J., Uyterlinde A.M., van Walsum M., Meijer C.J., Snow G.B., van Dongen G.A. (1993). MAb U36, a novel monoclonal antibody successful in immunotargeting of squamous cell carcinoma of the head and neck. Cancer Res.
16 Brakenhoff R.H., van Gog F.B., Looney J.E., van Walsum M., Snow G.B., van Dongen G.A. (1995). Construction and characterization of the chimeric monoclonal antibody E48 for therapy of head and neck cancer. Cancer Immunol Immunother.